# [^11^C]Acetoacetate

Chemical name: | [^11^C]Acetoacetate
Abbreviated name: | [^11^C]ACAC
Synonym: | [^11^C]Acetoacetic acid
Agent Category: | Compound
Target: | Acetoacetyl coenzyme A transferase and fatty acid synthetase
Target Category: | Incorporation into membrane
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Acetoacetate)]

Acetate is readily taken up by cells and is activated to acetyl-CoA in both the cytosol and mitochondria by acetyl-CoA synthetase. Acetyl-CoA is a common metabolic intermediate for synthesis of cholesterol and fatty acids, which are then incorporated into membrane tissue (1). Acetyl-CoA is oxidized in mitochondria by the tricarboxylic acid (TCA) cycle to carbon dioxide and water. Some of the acetate is converted to amino acids. In normal myocardium, acetate is metabolized to CO_2_via the TCA cycle as the dominant pathway. In contrast, tumor cells convert most of the acetate into fatty acids by a key enzyme fatty acid synthetase, which is overexpressed in cancer cells (2). Acetate is predominantly incorporated into intracellular phosphatidylcholine membrane microdomains that are important for tumor growth and metastasis (3). [^11^C]Acetate is used as a positron emission tomography (PET) tracer in the study of myocardial oxidative metabolism and regional myocardial blood flow (4). [^11^C]Acetate is a promising PET tracer for renal, pancreatic, and prostate tumors (5).

Under normal conditions, glucose is converted to acetate to feed into the TCA cycle for energy generation. However, ketone bodies (acetoacetate and hydroxybutyrate) are produced by the liver when the carbohydrate intake is low or during fasting. Liver cells do not utilize the ketone bodies because of a lack of acetoacetyl-CoA transferase for the metabolism of acetoacetate. The ketone bodies became the primary source of energy for the brain, heart, kidney, and skeletal muscle, where they are converted to acetyl-CoA. Human mammary carcinomas and rat hepatomas were found to express increased levels of acetoacetyl-CoA transferase activity in correlation with their growth rates (6, 7). [^11^C]Acetoacetate ([^11^C]ACAC ) is being evaluated as a PET agent to measure ketone body utilization by the tumors and brain (8, 9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Acetoacetate%20AND%20synthesis)]

[^11^C]ACAC was produced by a reaction of the enolate anion of acetone with [^11^C]carbon dioxide in tetrahydrofuran followed by hydrolysis (9). This method produced [^11^C]ACAC with a radiochemical yield of 24–58% (decay-corrected) in 30 min with a specific activity of 22.2 GBq/mmol (0.6 Ci/mmol) at the end of bombardment. The radiochemical purity of [^11^C]ACAC was found to be ~97%. An automated one-pot synthesis system provided radiochemical yields of 22–47% (decay-corrected, n = 20) and radiochemical purity of >97% in 18 min (10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Acetoacetate%20AND%20%22in%20vitro%22%5BMeSH%20Terms%5D)]

Authier et al. (8) compared [^11^C]ACAC and [^11^C]acetate uptake in two murine breast cancer cell lines MC7-L1 and MC4-L2 (8). For MC7-L1 cells, 65.5% and 53.0% of total radioactivity were in the cellular lipids at 60 min of incubation with [^11^C]ACAC and [^11^C]acetate, respectively. For MC4-L2 cells, 60.4% and 65.6% of total radioactivity accumulation of [^11^C] ACAC and [^11^C]acetate was found in the cellular lipids at 60 min of incubation, respectively. Therefore, both [^11^C]ACAC and [^11^C]acetate may be metabolized using the similar metabolic pathways leading to lipid synthesis.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Acetoacetate%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Authier et al. (8) studied the biodistribution of [^11^C]ACAC and [^11^C]acetate in mice bearing tumors of various cell lines (n = 2 - 10 mice/group). The optimal tumor accumulation of [^11^C]ACAC was between 5 and 30 min after injection, with maximal accumulation of 2.72 ± 0.38%, 2.42 ± 1.10%, 2.54 ± 0.87%, and 3.15 ± 0.58% ID/g for MC7-L1, MC4-L2, PC3, and LN-CaP tumors, respectively. The optimal tumor accumulation of [^11^C]acetate was reached at 5–15 min after injection, with maximal accumulation of 1.25 ± 0.05%, 2.30 ± 09%, and 0.96 ± 0.24% ID/g for MC7-L1, MC4-L2, and PC3, respectively. The tumor/muscle ratios and tumor accumulation tended to be higher for [^11^C]ACAC than [^11^C]acetate, but the differences did not reach statistical significance (P > 0.05). High to moderate accumulation was observed in the kidneys, spleen, liver, heart, lung, brain, and ovaries/testes for both tracers. Prenen et al. (9) performed PET imaging to study tissue accumulation of [^11^C]ACAC in rats (n = 6) at 20 min after injection. The organ with the highest uptake was the liver (3.6 ± 0.5% injected dose (ID)), followed by the brain (2.7 ± 0.4% ID), kidneys (2.5 ± 0.4% ID), and heart (2.0 ± 0.5% ID).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Acetoacetate%20AND%20%22animals%22%5BMeSH%5D%20NOT%20%22rodentia%22%5BMeSH%20Terms%5D%20NOT%20%22primates%22%5BMeSH%5D)]

Prenen et al. (9) performed PET imaging to study tissue accumulation of [^11^C]ACAC in cats (n = 2) at 1.5-20 min after injection. The organ with the highest uptake was the liver (8.5-12.7% ID), followed by the brain (6.6-10.4% ID), kidneys (4.8-6.6% ID), and heart (2.3-2.95% ID) at 20 min.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Acetoacetate%20AND%20%22primates%22%5BMeSH%5D%20NOT%20%22humans%22%5BMeSH%5D)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Acetoacetate%20AND%20%22humans%22%5BMeSH%20Terms%5D)]

No publication is currently available.

## References

1 Howard B.V., Howard W.J. (1975). Lipids in normal and tumor cells in culture. Prog Biochem Pharmacol.
2 Swinnen J.V., Heemers H., Deboel L., Foufelle F., Heyns W., Verhoeven G. (2000). Stimulation of tumor-associated fatty acid synthase expression by growth factor activation of the sterol regulatory element-binding protein pathway. Oncogene.
3 Swinnen J.V., Van Veldhoven P.P., Timmermans L., De Schrijver E., Brusselmans K., Vanderhoydonc F., Van de Sande T., Heemers H., Heyns W., Verhoeven G. (2003). Fatty acid synthase drives the synthesis of phospholipids partitioning into detergent-resistant membrane microdomains. Biochem Biophys Res Commun.
4 Visser F.C. (2001). Imaging of cardiac metabolism using radiolabelled glucose, fatty acids and acetate. Coron Artery Dis.
5 Schoder H., Larson S.M. (2004). Positron emission tomography for prostate, bladder, and renal cancer. Semin Nucl Med.
6 Fenselau A., Wallis K., Morris H.P. (1976). Subcellular localization of acetoacetate coenzyme A transferase in rat hepatomas. Cancer Res.
7 Kallinowskil F., Davel S., Vaupell P., Baessler K.H., Wagner K. (1985). Glucose, lactate, and ketone body utilization by human mammary carcinomas in vivo. Adv Exp Med Biol.
8 Authier S., Tremblay S., Dumulon V., Dubuc C., Ouellet R., Lecomte R., Cunnane S.C., Benard F. (2008). [(11)C] Acetoacetate Utilization by Breast and Prostate Tumors: a PET and Biodistribution Study in Mice. Mol Imaging Biol.
9 Prenen G.H., Go K.G., Zuiderveen F., Paans A.M., Vaalburg W. (1990). An improved synthesis of carbon-11 labeled acetoacetic acid and an evaluation of its potential for the investigation of cerebral pathology by positron emission tomography. Int J Rad Appl Instrum [A].
10 Tremblay S., Ouellet R., Rodrigue S., Langlois R., Benard F., Cunnane S.C. (2007). Automated synthesis of 11C-acetoacetic acid, a key alternate brain fuel to glucose. Appl Radiat Isot.